# ^99m^Tc-Labeled anti-macrophage mannose receptor (MMR; CD206) nanobody

Chemical name: | ^99m^Tc-Labeled anti-macrophage mannose receptor (MMR; CD206) nanobody
Abbreviated name: | [^99m^Tc]MMR Nb
Synonym:
Agent Category: | Antibody
Target: | Macrophage mannose receptor (CD206)
Target Category: | Receptor
Method of detection: | Single-photon emission computed tomography (SPECT); gamma planar imaging
Source of signal / contrast: | ^99m^Tc
Activation: | No
Studies: | - In vitro; - Rodents | Structure not available in PubChem (http://www.ncbi.nlm.nih.gov/pcsubstance).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=macrophage%20mannose%20receptor&cmd=DetailsSearch)]

Cancerous tumors consist of transformed cells that are surrounded by stromal cells (or healthy, normal host cells) consisting of cells such as the fibroblasts, endothelial cells, various myeloid cells, and the extracellular matrix (1). The various cell types in the tumor interact with each other constantly so as to maintain homeostasis in the lesion. In a cancerous tumor, the stromal cells produce ligands that assist in the maintenance and growth of the tumor (e.g., by inducing angiogenesis), and the neoplastic cells reciprocate by generating factors that help in the survival, growth, and proliferation of the stromal cells (2). In addition, a large number of macrophages infiltrate and reside in the tumor stroma (known as tumor-associated macrophages; TAMs), and these cells are also known to promote growth and proliferation of the tumor because they produce factors that are inflammatory, pro-angiogenic, and immunosuppressive, and that assist in the metastasis of the cancer (3). On the basis of their gene and protein expression profile, two distinct types of TAMs are found in the tumor stroma. The TAMs either have a low expression of the major histocompatibility complex class II (MHC II) (MHC^low^ TAMs) or express high levels of MHC II (MHC^hi^ TAMs). The MHC^low^ TAMs are present mainly in the hypoxic areas of the tumor, are strong promoters of angiogenesis, and overexpress the macrophage mannose receptor (MMR, CD206), an endocyte C-type lectin receptor (3). The MHC^hi^ TAMs are found primarily in the perivascular regions of a cancerous lesion and exhibit a low angiogenic potential (3). Therefore, MMR could be a valuable target for the noninvasive imaging of MMR^+^ stromal cells with single-photon emission computed tomography (SPECT) to visualize tumor stroma, and the stromal cells could be targeted to treat neoplastic lesions.

There is a great deal of interest to develop imaging probes that are based on a nanobody (Nb) scaffold because Nbs are miniature antibodies (Ab) (~15 kDa compared with ~150 kDa for a normal Ab) that are rapidly eliminated through the kidneys and, if labeled with a radionuclide, generate a high signal/noise ratio at the target site (4). To learn about the unique source, structure, properties, and application of Nbs, see Vaneycken et al. (5). Movahedi et al. generated an anti-MMR Nb, labeled it with ^99m^Tc, and showed that the radiolabeled Nb ([^99m^Tc]MMR Nb) can be used to detect MMR^+^ stromal cells with SPECT in mice bearing either TS/A cell tumors (a mouse mammary adenocarcinoma cell line) or 3LL-R cell tumors (a C57BL/6 Lewis lung carcinoma cell line) (3, 4).

### Related Resource Links

Nanobody-related chapters in MICAD (http://www.ncbi.nlm.nih.gov/books/?term=Nanobodies+AND+micad%5Bbook%5D&view=chapter&p%24a=&p%24l=PBooksLayout&p%24st=books)

Nanobodies in clinical trials (http://clinicaltrials.gov/ct2/results?term=Nanobody)

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=Anti-MMR%20nanobody%20synthesis&cmd=DetailsSearch)]

Two anti-MMR Nbs, Nb cl1 and Nb cl2 (with a hexahistidine tag on the C-terminus to facilitate labeling with a radionuclide), were generated against the extracellular domain of the MMR. The Nbs were expressed and purified from a bacterial expression system as described elsewhere (4). Bivalent Nbs (biv Nbs), designated Nb biv (G_4_S)_3_, Nb biv IgG2c, and Nb biv IgA, which contained different types of linkers (for details regarding the linkers and the biv Nbs, see Movahedi et al. (4)), were also generated for use in some studies. The various Nbs were radiolabeled with ^99m^Tc at their H_6_ tails, as described by Vaneycken et al. (6). For use as a negative control, another Nb, Bcll10, which is directed against the β-lactamase (7), was also labeled with ^99m^Tc. The radiochemical yield, radiochemical purity, specific activity, and stability of the different Nb or biv Nb probes were not reported.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=Anti-MMR%20nanobody%20in%20vitro&cmd=DetailsSearch)]

Surface plasmon resonance (SPR) measurements with Nb cl1 and Nb cl2 showed that Nb cl1 had an 8-fold higher affinity (K_D_ = 2.31 × 10−^8^ mol/L) for MMR compared with Nb cl2 (K_D_ = 1.91 × 10−^7^ mol/L) (4). In addition, it was shown that the two Nbs did not bind to the same epitope on the MMR (4). The MMR binding affinities of Nb biv (G_4_S)_3_, Nb biv IgG2c, and Nb biv IgA were reported to be 4.22 × 10−^9^ mol/L, 4.04 × 10−^9^ mol/L, and 4.69 × 10−^9^ mol/L, respectively, as determined with SPR.

Flow cytometric analysis showed that fluorescence-labeled Nb cl1 bound only to the CD11b^+^ and not to the CD11^–^ cell fractions of single-cell suspensions derived from either the TS/A tumors or the 3LL-R tumors (4). In addition, the fluorescent Nb bound largely to the MHC^low^ TAMs in the TS/A cells, whereas the binding was restricted to the MHC^low^ TAMs with the 3LL-R cells.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=Anti-MMR%20nanobody%20rodentia&cmd=DetailsSearch)]

Biodistribution and SPECT/micro-computed tomography (micro-CT) imaging studies with the different types of ^99m^Tc-labeled Nbs were performed in naïve wild-type (WT) mice, MMR knockout (MMR-KO) mice, and chemokine receptor 2 knockout (CCR2-KO), mice as described by Movahedi et al. (4). The animals were injected intravenously with 45–155 MBq (1.66–5.73 mCi) of the ^99m^Tc-labeled Nbs in the presence or absence of an excess amount (quantity not reported) of an unlabeled Nb or a biv Nb. Whole-body SPECT images were acquired from the animals at 60 min or 180 min postinjection (p.i.); at 30 min after acquiring the images, the animals were euthanized to determine the amount of accumulated radioactivity in the various organs of interest. Data were presented as percent of injected activity per gram tissue (% IA/g).

Groups of naïve WT mice (number of animals per group was not reported) were injected with either [^99m^Tc]Nb cl1, [^99m^Tc]Nb cl2, or [^99m^Tc]NbBCII10 (control) to determine if the ^99m^Tc-labeled Nbs were suitable for the imaging of organs that express MMR under in vivo conditions (e.g., the liver and the spleen) (4). Whole-body SPECT/micro-CT images were acquired from the animals at 60 min p.i., and the images showed that the radioactivity from all three probes was present primarily in the kidneys and the urinary bladder of the animals. The images showed that the accumulation of radioactivity with [^99m^Tc]Nb cl1 and [^99m^Tc]Nb cl2 was mainly in the liver and spleen of the animals. However, animals injected with [^99m^Tc]NbBCII10 showed no accumulation of label in these organs. Ex vivo analysis of the various organs obtained from these animals showed that, with [^99m^Tc]Nb cl1 and [^99m^Tc]Nb cl2, the amount of radioactivity present in the liver was 15.55 ± 0.54% IA/g and 7.92 ± 0.42% IA/g, respectively, and the amount of radioactivity in the spleen was 6.79 ± 0.08% IA/g and 3.97 ± 0.65% IA/g, respectively. All other organs, such as the heart, lungs, and bone, showed an uptake of 1%–2.5% IA/g. With [^99m^Tc]NbBCII10, all the organs, including the liver and the spleen, showed an uptake of <1% IA/g. The biodistribution of [^99m^Tc]Nb cl1, [^99m^Tc]Nb cl2, and [^99m^Tc]NbBCII10 in MMR-KO mice was observed to be similar to that of [^99m^Tc]NbBCII10 in the WT rodents. From this study, the investigators concluded that the cl1 and cl2 Nbs have a high in vivo specificity to target organs that express the MMR. The investigators selected Nb cl1 for any further work because it exhibited a higher in vitro affinity for the MMR, and the in vivo uptake of radioactivity in the various organs was higher with this Nb compared with Nb cl2.

In another study, WT mice (number of animals was not reported) bearing TS/A cell and 3LL-R cell subcutaneous tumors were injected with [^99m^Tc]Nb cl1 as before. SPECT/micro-CT images of the animals acquired at 3 h p.i. showed that the lesions were clearly visible at this time point (4). In comparison, the tumors showed very little uptake of radioactivity from the radiolabeled control Nb ([^99m^Tc]BCll10). Ex vivo analysis of the TS/A and 3LL-R tumors showed that the uptake of label from [^99m^Tc]Nb cl1 in the lesions was 3.02 ± 0.10% IA/g and 3.02 ± 0.19% IA/g, respectively, compared with an accumulation of 0.40 ± 0.03% IA/g and 0.74 ± 0.03% IA/g, respectively, with [^99m^Tc]BCll10 (4). In addition, the accumulation of radioactivity from [^99m^Tc]Nb cl1 in the 3LL-R tumors in MMR-KO mice was 10-fold less (0.33 ± 0.03% IA/g) compared with the lesions in the WT rodents, indicating that the uptake of radioactivity in the tumors was dependent on the expression of MMR by the host stromal cells (4).

It was shown that low expression of CCR2 in a tumor can significantly reduce the infiltration of TAMs into the lesion; however, CCR2-deficiency does not affect the growth of the neoplasm (4). To ascertain that [^99m^Tc]Nb cl1 targeted only TAMs in the tumors, WT mice and CCR2-KO mice (number of animals per group was not reported) bearing 3LL-R cell tumors were injected with the ^99m^Tc-labeled Nb, and the amount of tracer that accumulated in the lesions from the two groups of animals was determined. Tumors from the WT mice showed an accumulation of 2.97 ± 0.22% IA/g, which was significantly higher (P value not reported) than the uptake of 1.83 ± 0.1% IA/g observed in the tumors of the CCR2-KO mice (4). This observation suggested that Nb cl1 specifically targeted the TAMs in the cancerous lesions (4).

The biodistribution patterns of the ^99m^Tc-labeled bivalent Nbs ([^99m^Tc]Nb biv (G_4_S)_3_, [^99m^Tc]Nb biv IgG2c, and [^99m^Tc]Nb biv IgA) were investigated in WT mice bearing TS/A and 3LL-R tumors (4). From SPECT/micro-CT images, it was clear that the label from the bivalent Nbs accumulated mainly the liver and the spleen, but little uptake of the label was observed in the tumors compared with the monovalent cl1 Nb. From this study, the investigators concluded that the bivalent Nbs primarily blocked the extratumoral binding sites in the animals and had little affinity for the intratumoral binding sites. To test this hypothesis, [^99m^Tc]Nb cl1 was coinjected with 20-fold excess nonradioactive bivalent Nb (amount not reported) in mice bearing subcutaneous TS/A cell tumors, and SPECT/micro-CT images were acquired at 3 h p.i (4). From the images it was apparent that the incorporation of radioactivity in all the organs was reduced to background levels, i.e., the uptake of label was comparable to that observed with [^99m^Tc]BCll10, and maximum uptake of radioactivity was observed in the tumors of the rodents.

Imaging studies were performed to evaluate the use of [^99m^Tc]Nb cl1 for the visualization of microscopic mammary tumors in MMTV-PyVT (http://jaxmice.jax.org/strain/002374.html) transgenic mice, which develop the lesions spontaneously (4). For this, mice (n = 3 animals/group) bearing multiple microscopic tumors were injected with [^99m^Tc]BCll10, [^99m^Tc]Nb cl1, or a mixture of [^99m^Tc]Nb cl1 and 20-fold excess nonradioactive biv Nb cl1 at 48-h intervals (to allow for complete decay of the radionuclide). Whole-body SPECT/micro-CT images were acquired from the animals at 3 h p.i. The tumors could not be distinguished easily from the organs in the images obtained from mice injected with [^99m^Tc]Nb cl1 alone, but the tumors were clearly visible in the images from animals injected with a mixture of [^99m^Tc]Nb cl1 and the biv Nb cl1. In addition, fluorescence-activated cell-sorting analysis of cells from three select tumors showed the presence of distinct subpopulations of MHC^low^ TAMs that expressed the MMR.

From these studies, the investigators concluded that the ^99m^Tc-labeled MMR Nbs can be used for the targeted imaging of cancerous tumors in rodents (4).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=Anti-MMR%20nanobody%20Other%20Non-Primate%20Mammals&cmd=DetailsSearch)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=Anti-MMR%20nanobody%20Non-Human%20Primates&cmd=DetailsSearch)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=Anti-MMR%20nanobody%20Human%20Studies&cmd=DetailsSearch)]

No publication is currently available.

## Supplemental Information

[Disclaimers]

No information is currently available.

## References

1 Briest F., Berndt A., Clement J., Junker K., Eggeling F., Grimm S., Friedrich K. (2012). Tumor-stroma interactions in tumorigenesis: lessons from stem cell biology. Front Biosci.
2 Engels B., Rowley D.A., Schreiber H. (2012). Targeting stroma to treat cancers. Semin Cancer Biol.
3 Movahedi K., Laoui D., Gysemans C., Baeten M., Stange G., Van den Bossche J., Mack M., Pipeleers D., In't Veld P., De Baetselier P., Van Ginderachter J.A. (2010). Different tumor microenvironments contain functionally distinct subsets of macrophages derived from Ly6C(high) monocytes. Cancer Res.
4 Movahedi K., Schoonooghe S., Laoui D., Houbracken I., Waelput W., Breckpot K., Bouwens L., Lahoutte T., De Baetselier P., Raes G., Devoogdt N., Van Ginderachter J.A. (2012). Nanobody-based targeting of the macrophage mannose receptor for effective in vivo imaging of tumor-associated macrophages. Cancer Res.
5 Vaneycken I., D'Huyvetter M., Hernot S., De Vos J., Xavier C., Devoogdt N., Caveliers V., Lahoutte T. (2011). Immuno-imaging using nanobodies. Curr Opin Biotechnol.
6 Vaneycken I., Govaert J., Vincke C., Caveliers V., Lahoutte T., De Baetselier P., Raes G., Bossuyt A., Muyldermans S., Devoogdt N. (2010). In vitro analysis and in vivo tumor targeting of a humanized, grafted nanobody in mice using pinhole SPECT/micro-CT. J Nucl Med.
7 Conrath K.E., Lauwereys M., Galleni M., Matagne A., Frere J.M., Kinne J., Wyns L., Muyldermans S. (2001). Beta-lactamase inhibitors derived from single-domain antibody fragments elicited in the camelidae. Antimicrob Agents Chemother.